# ^111^In-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-conjugated monomeric [Tyr^3^]octreotide

Chemical name: | ^111^In-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-conjugated monomeric [Tyr^3^]octreotide
Abbreviated name: | ^111^In-Monomeric [Tyr^3^]octreotide
Synonym:
Agent Category: | Peptides
Target: | Somatostatin receptors (SSTRs)
Target Category: | Receptors
Method of detection: | Single-photon emission computed tomography (SPECT) and planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | For structures of octreotide analogues, click on PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance?term=octreotide).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=somatostatin+receptor+and+targeted)]

The ^111^In-labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA)-conjugated monomeric [Tyr^3^]octreotide, abbreviated as ^111^In-monomeric [Tyr^3^]octreotide, is an octreotide-based agent developed by Yim et al. for somatostatin receptor (SSTR)–targeted imaging and radionuclide therapy (1).

The human SSTR family is a group of G-protein–coupled receptors with five members (SSTR1–SSTR5). All receptor members have seven α-helical transmembrane domains and possess a highly conserved sequence motif (YANSCANPI/VLY) in the seventh topology, which serves as a signature sequence for this family (2-4). Overall, there is 39%–57% sequence identity among the members, with the highest homology between SSTR1 and SSTR4, and among SSTR2, SSTR3, and SSTR5, respectively. The two groups of receptors also differ in their interactions with somatostatin (SST) and its analogs (1, 3-5). SSTR2, SSTR3, and SSTR5 have a high affinity for octreotide and seglitide, whereas SSTR1 and SSTR4 exhibit a very low affinity for them. SSTRs are distributed widely in cells both in the nervous system and periphery, and they have been shown to be overexpressed in a large number of malignancies, with particularly high density in neuroendocrine tumors (2, 6, 7).

As the targets of SST radiopharmaceuticals, SSTRs are of considerable clinical relevance for tumor imaging and radionuclide therapy (2, 8, 9). Because the native SST has a very short biological half-life (<2 min), various analogs have been synthesized, including octreotide, lanreotide, vapreotide, and their derivatives (4, 9, 10). In general, these analogs have a high affinity to SSTR2, somewhat lower affinity to SSTR3 and SSTR5, and almost no affinity to SSTR1 and SSTR4. Treatment with the radiolabeled analogs results in reduced hormonal overproduction and symptomatic relief in most patients with neuroendocrine tumors; however, it is much less successful in tumor size reduction (11, 12). Imaging with ^111^In-, ^90^Y-, or ^177^Lu-labeled [DOTA^0^,Tyr^3^]octreotide analogs has proven the usefulness of octreotide conjugates in the diagnosis and staging of neuroendocrine tumors (7-9, 13).

There is growing interest in the development of polyvalent ligands for dual imaging and therapeutic purposes, considering that polyvalent ligands may have a higher binding affinity than monovalent analogs (1). Yim et al., synthesized mono-, di-, and tetrameric [Tyr^3^]octreotide conjugates with a two-stage metal-free ligation procedure (1). The investigators characterized these conjugates and compared them with ^111^In-labeled [DOTA^0^,Tyr^3^]octreotide ([^111^In-DOTA^0^,Tyr^3^]octreotide), a chemically engineered and long-acting analog. [^111^In-DOTA^0^,Tyr^3^]octreotide has been applied for imaging and treatment in patients with neuroendocrine tumors (9, 11, 12). Yim et al. have shown that the ^111^In-labeled monomeric and dimeric [Tyr^3^]octreotides, but not the ^111^In-labeled tetrameric [Tyr^3^]octreotide, have a similar binding affinity for SSTRs and a longer tumor retention time when compared with [^111^In-DOTA^0^,Tyr^3^]octreotide (1). This chapter describes the results obtained with ^111^In-monomeric [Tyr^3^]octreotide.

### Related Resource Links:

- MICAD chapters on SSTR imaging (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=somatostatin+receptor+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information on SSTRs (http://www.ncbi.nlm.nih.gov/gene/?term=somatostatin+receptors)
- Articles on SSTRs in Online Mendelian Inheritance in Man (OMIM (http://www.ncbi.nlm.nih.gov/omim?term=somatostatin%20receptors))
- Somatostatin analogs in PubChem (http://www.ncbi.nlm.nih.gov/sites/entrez?db=pccompound&term=somatostatin)
- Bioassays of SSTRs in PubChem (http://www.ncbi.nlm.nih.gov/pcassay?term=somatostatin%20receptors)
- SSTR-related clinical trials in ClinicalTrial.gov (http://clinicaltrials.gov/ct2/results?term=somatostatin+receptors)
- FDA-approved octreotide agents: Octreotide acetate (http://www.accessdata.fda.gov/scripts/cder/drugsatfda/index.cfm) and Octreoscan (http://www.accessdata.fda.gov/scripts/cder/drugsatfda/index.cfm?fuseaction=Search.DrugDetails)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20411957)]

DOTA-Conjugated monomeric [Tyr^3^]octreotide was synthesized with a two-stage ligation procedure that combined the Cu(I)-catalyzed “click” reaction between dendrimeric alkynes and peptidic azides and the subsequent copper-free thio acid/azide “sulfo-click” amidation reaction between the obtained dendrimeric peptide thio acids and a DOTA-derived sulfonyl azide (1). The ^111^In-labeling was achieved in NH_4_OAc buffer (pH 5.5) with ^111^InCl_3_ by heating the reaction mixture for 10–15 min at 95ºC. The radiochemical yield of the ^111^In-monomeric [Tyr^3^]octreotide was >98% with a specific activity of 13.6 GBq/μmol (0.37 Ci/μmol). Its lipophilicity, expressed as log(D) value, was −2.20 ± 0.17, 25-fold higher than that of [^111^In-DOTA^0^,Tyr^3^]octreotide (−3.59 ± 0.14). This could be attributed to the aromatic character of the dendrimer-derived linker moiety.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20411957)]

Binding affinity of the monomeric [Tyr^3^]octreotide for SSTRs was determined using SSTR2-expressing AR42J tumor cells in a competitive binding assay (1). [^111^In-DOTA^0^,Tyr^3^]octreotide was used as a radiotracer, and commercially available [DOTA^0^,Tyr^3^]octreotide was included as a competing ligand. The monomeric [Tyr^3^]octreotide had a 50% inhibition concentration (IC_50_) of 1.32 nM, better than that of the reference [DOTA^0^,Tyr^3^]octreotide (IC_50_ = 2.45 nM). The IC_50_ values for the dimeric and tetrameric [Tyr^3^]octreotide conjugates were 2.45 nM and 14.0 nM, respectively. These results showed a decreased binding affinity with increased valency. The hypothesized increase in receptor affinity due to multimerization was not observed, especially in the case of tetrameric [Tyr^3^]octreotide, which may be attributed to the limited water solubility of the [Tyr^3^]octreotide conjugates. The IC_50_ values for all ^111^In-labeled conjugates improved by a factor of 1.4–2.9, compared to unlabeled counterparts.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20411957)]

In vivo biodistribution and tumor targeting of ^111^In-monomeric [Tyr^3^]octreotide were investigated in BALB/c nude mice bearing subcutaneous AR42J tumors (n = 5 mice/time point) (1). [^111^In-DOTA^0^,Tyr^3^]octreotide was used as the reference compound, with a tumor uptake of 19.5 ± 4.84% injected dose per gram tissue (ID/g) at 2 h and 7.47 ± 0.78% ID/g at 24 h after tail vein injection. ^111^In-Monomeric [Tyr^3^]octreotide exhibited a rapid and high tumor uptake with 42.33 ± 2.80% ID/g at 2 h and 10.75 ± 2.98% ID/g at 24 h after injection. The tumor uptake was blocked with co-injection of excess octreotide (50 µg, n = 3 mice) (4.82 ± 0.87% ID/g at 2 h). The blood clearance of ^111^In-monomeric [Tyr^3^]octreotide was fast (0.27 ± 0.03% ID/g at 2 h and 0.04 ± 0.01% ID/g at 24 h), with the tumor/blood ratios increasing from 156 ± 18.9 at 2 h to 268 ± 104 at 24 h after injection. Among the organs, the kidney had the highest uptake with 54.19 ± 7.44% ID/g and 2.53 ± 0.67% ID/g at 2 h and 24 h, respectively. Low uptake was observed in the pancreas, stomach, and colon. The higher tumor uptake of ^111^In-monomeric [Tyr^3^]octreotide compared to [^111^In-DOTA^0^,Tyr^3^]octreotide emphasizes the importance of the implemented sulfonamide linker and dendrimer-derived core for tumor targeting.

^111^In-Dimeric [Tyr^3^]octreotide (refer to MICAD chapter for details (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html)) exhibited behavior similar to ^111^In-monomeric [Tyr^3^]octreotide, whereas ^111^In-tetrameric [Tyr^3^]octreotide behaved differently than its monomeric and dimeric counterparts. ^111^In-Tetrameric [Tyr^3^]octreotide had high uptake in the liver and spleen but negligible tumor accumulation. Tetramerization of the [Tyr^3^]octreotide had profound implications on its lipophilicity and consequently on receptor affinity and tumor uptake.

In conclusion, the IC_50_ values of mono- and multimeric [Tyr^3^]octreotide conjugates are all in the low nanomolar range. Monomeric [Tyr^3^]octreotide has the highest binding affinity for SSTRs, followed by dimeric [Tyr^3^]octreotide and tetrameric [Tyr^3^]octreotide. In mouse models, ^111^In-monomeric [Tyr^3^]octreotide has the highest tumor uptake, better than that of the [^111^In-DOTA^0^,Tyr^3^]octreotide, whereas ^111^In-dimeric [Tyr^3^]octreotide exhibits the longest tumor retention, probably due to the bivalency effect. Both monomeric and dimeric [Tyr^3^]octreotide conjugates exhibit interesting properties for imaging and therapeutic applications (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Yim C.B., Dijkgraaf I., Merkx R., Versluis C., Eek A., Mulder G.E., Rijkers D.T., Boerman O.C., Liskamp R.M. (2010). Synthesis of DOTA-conjugated multimeric [Tyr3]octreotide peptides via a combination of Cu(I)-catalyzed "click" cycloaddition and thio acid/sulfonyl azide "sulfo-click" amidation and their in vivo evaluation. J Med Chem.
2 Froidevaux S., Eberle A.N. (2002). Somatostatin analogs and radiopeptides in cancer therapy. Biopolymers.
3 Tulipano G., Schulz S. (2007). Novel insights in somatostatin receptor physiology. Eur J Endocrinol.
4 van der Hoek J., Hofland L.J., Lamberts S.W. (2005). Novel subtype specific and universal somatostatin analogues: clinical potential and pitfalls. Curr Pharm Des.
5 Lesche S., Lehmann D., Nagel F., Schmid H.A., Schulz S. (2009). Differential effects of octreotide and pasireotide on somatostatin receptor internalization and trafficking in vitro. J Clin Endocrinol Metab.
6 Strowski M.Z., Blake A.D. (2008). Function and expression of somatostatin receptors of the endocrine pancreas. Mol Cell Endocrinol.
7 Kwekkeboom D.J., Kam B.L., van Essen M., Teunissen J.J., van Eijck C.H., Valkema R., de Jong M., de Herder W.W., Krenning E.P. (2010). Somatostatin-receptor-based imaging and therapy of gastroenteropancreatic neuroendocrine tumors. Endocr Relat Cancer.
8 Bal C.S., Gupta S.K., Zaknun J.J. (2010). Radiolabeled somatostatin analogs for radionuclide imaging and therapy in patients with gastroenteropancreatic neuroendocrine tumors. Trop Gastroenterol.
9 de Jong M., Breeman W.A., Kwekkeboom D.J., Valkema R., Krenning E.P. (2009). Tumor imaging and therapy using radiolabeled somatostatin analogues. Acc Chem Res.
10 Ferone D., Saveanu A., Culler M.D., Arvigo M., Rebora A., Gatto F., Minuto F., Jaquet P. (2007). Novel chimeric somatostatin analogs: facts and perspectives. Eur J Endocrinol.
11 Kwekkeboom D.J., Mueller-Brand J., Paganelli G., Anthony L.B., Pauwels S., Kvols L.K. (2005). M. O'Dorisio T, R. Valkema, L. Bodei, M. Chinol, H.R. Maecke, and E.P. Krenning, Overview of results of peptide receptor radionuclide therapy with 3 radiolabeled somatostatin analogs. J Nucl Med.
12 Hofland, L.J., J. van der Hoek, R. Feelders, A.J. van der Lely, W. de Herder, and S.W. Lamberts, Pre-clinical and clinical experiences with novel somatostatin ligands: advantages, disadvantages and new prospects. J Endocrinol Invest, 2005. 28(11 Suppl International): p. 36-42.
13 Gerasimou G., Moralidis E., Gotzamani-Psarrakou A. (2010). Somatostatin receptor imaging with (111)In-pentetreotide in gastro-intestinal tract and lung neuroendocrine tumors-Impact on targeted treatment. Hell J Nucl Med.
14 Mintzer, M.A. and M.W. Grinstaff, Biomedical applications of dendrimers: a tutorial. Chem Soc Rev, 2010